# N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^131^I]iodo-5-methoxybenzyl)acetamide

Chemical name: | N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^131^I]iodo-5-methoxybenzyl)acetamide
Abbreviated name: | [^131^I]PBR3a
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+3a)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as the central benzodiazepine receptor (CBR) and the peripheral benzodiazepine receptor (PBR). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR-antagonistic activity. [^11^C]PK11195 is being developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET probes with highly selective and specific binding to PBR. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^131^I]iodo-5-methoxybenzyl)acetamide ([^131^I]PBR3a), a DAA1106 analog, has been developed for single-photon emission computed tomography (SPECT) imaging of PBR in the brain.

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+3a+synthesis)]

In the report by Zhang et al. (10), [^131^I]PBR3a was synthesized by ^131^I-iodination of the tributylstannyl precursor with [^131^I]NaI in the presence of H_2_O_2_ in acetic acid. [^131^I]PBR3a was purified with high-performance liquid chromatography for a radiochemical yield of >80%. The specific activity was >30 GBq/μmol (0.81 Ci/μmol) at the end of synthesis with >98% radiochemical purity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+3a+in+vitro)]

In vitro quantitative autoradiography with [^11^C]DA1106 on rat brain sections showed that PBR3a had an inhibition concentration (IC_50_) value of 7.8 ± 0.4 nM, which is slightly lower than DA1106 (IC_50_ = 1.6 ± 0.1 nM) and similar to PK11195 (IC_50_ = 8.3 ± 1.2 nM) (10). PBR3a has an IC_50_ value of >10,000 nM on CBR as measured by ^11^C-labeled flumazenil binding in the rat brain sections. PBR3a has a logD value of 4.42.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+3a+rodentia)]

Zhang et al. (10) reported biodistribution studies of [^131^I]PBR3a in mouse brains (n = 3 per group) that showed rapid accumulation of radioactivity with 1.06% injected dose per gram (ID/g) at 1 min, 1.36% ID/g at 5 min, 1.69% ID/g at 15 min, 1.28% ID/g at 30 min, and 0.75% ID/g at 60 min. Regional brain accumulation showed that the highest radioactivity level was in the olfactory bulb (3.06% ID/g), followed by the cerebellum (2.32% ID/g), hypothalamus (0.97% ID/g), cortex (0.84% ID/g), hippocampus (0.75% ID/g), striatum (0.69% ID/g), and thalamus (0.48% ID/g) at 15 min. The level of radioactivity in the blood was 1.11% ID/g at 15 min and 0.25% ID/g at 60 min. At 30 min after injection, 90–94% of total brain radioactivity was intact [^131^I]PBR3a. Co-injection of [^131^I]PBR3a with DAA1106 or PK11195 (1 mg/kg) decreased the accumulation in the olfactory bulb and cerebellum by 60–67% at 30 min after injection and to a lesser extent (10–30%) in the hypothalamus, cortex, hippocampus, striatum, and thalamus. Ex vivo autoradiography studies found the highest level of radioactivity in the choroid plexus in addition to the olfactory bulb and cerebellum at 30 min after injection. Co-injection of PK11195 clearly reduced radioactivity in the choroid plexus and olfactory bulb by 57% and in the cerebellum by 37%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+3a+(dog+or+pig+or+sheep+or+rabbit))]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+3a+(primate+not+human))]

No publications are currently available.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+3a+human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Zhang M.R., Kumata K., Maeda J., Haradahira T., Noguchi J., Suhara T., Halldin C., Suzuki K. (2007). N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[(131)I]iodo-5-me thoxybenzyl)acetamide: a potent iodinated radioligand for the peripheral-type benzodiazepine receptor in brain. J Med Chem.